# 3-(2-(S)-3,4-Dehydropyrrolinyl methoxy)-5-(3'-[^18^F]fluoropropyl)pyridine

Chemical name: | 3-(2-(S)-3,4-Dehydropyrrolinyl methoxy)-5-(3'-[^18^F]fluoropropyl)pyridine
Abbreviated name: | [^18^F]Nifrolene
Synonym:
Agent category: | Compound
Target: | α4β2 nicotinic acetylcholine receptor (nAChR)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20nifrolene)]

Neuronal nicotinic acetycholinergic receptors (nAChRs) are a heterogeneous family of ligand-gated ion channels expressed in the central nervous system, where their activation by acetylcholine and nicotine causes a rapid increase in cellular permeability to ions such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α (α2–α10) and four subtypes of structural β (β2–β5). nAChRs have been demonstrated to be involved in cognitive processes such as learning, memory, and control of movement in normal subjects. Dysfunction of nAChRs has been implicated in a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease, and Parkinson's disease. nAChRs also play a significant role in nicotine addiction.

The nAChR agonists 2-[^18^F]Fluoro-A-85380 and 6-[^18^F]Fluoro-A-85380 (2-[^18^F]FA (http://www.ncbi.nlm.nih.gov/books/NBK23401/) and 6-[^18^F]FA (http://www.ncbi.nlm.nih.gov/books/NBK23587/)) have been evaluated as positron emission tomography (PET) agents for the noninvasive study of nAChR in humans (4, 5). However, prolonged imaging times (2–4 h) are required for reliable quantification because of the slow kinetics of nAChR binding. 5-(3'-Fluoropropyl)-3-(2-(S)-pyrrolidinylmethoxy)pyridine (nifrolidine) is a putative and selective nAChR antagonist with nanomolar affinity. An antagonist may provide additional and complementary information about nAChR beyond that obtained with an agonist-based radiotracer such as 2-[^18^F]FA. For example, an antagonist will measure total receptor activity, whereas an agonist will measure the high-affinity receptor. 5-(3'-[^18^F]-Fluoropropyl)-3-(2-(S)-pyrrolidinylmethoxy)pyridine ([^18^F]nifrolidine) is being developed as a PET agent with faster kinetics than 2-[^18^F]FA and 6-[^18^F]FA for the noninvasive study of nAChR in the brain (6). Pichika et al. (7) replaced the pyrolidine ring in [^18^F]nifrolidine with 3,4-dehydroproline to produce 3-(2-(S)-3,4-dehydropyrrolinyl methoxy)-5-(3'-[¹⁸F]fluoropropyl)pyridine ([^18^F]nifrolene), which might have faster in vivo binding kinetics than[^18^F]nifrolidine.

### Related Resource Links:

- Chapters in MICAD (nACHR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=nAChR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (nicotinic α4 (http://www.ncbi.nlm.nih.gov/gene/1137), nicotinic β2 (http://www.ncbi.nlm.nih.gov/gene/1141))
- Articles in Online Mendelian Inheritance in Man (OMIM) (nicotinic α4 (http://omim.org/entry/118504), nicotinic β2 (http://omim.org/entry/118507))
- Clinical trials (nAChR (http://www.clinicaltrials.gov/ct2/results?term=nAChR))
- Drug information in FDA (nAChR (http://google2.fda.gov/search?q=Neuronal+nicotinic+acetylcholine+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20nifrolene%20and%20synthesis)]

Pichika et al. (7) reported the synthesis of [^18^F]nifrolene in a two-step reaction, which consisted of standard ^18^F-nucleophilic fluorination of 3-(1-tert-butoxycarbonyl-2-(S)-3,4-dehydropyrrolinylmethoxy)-5-(3-(4-methylsulfonyloxy)-propyl)pyridine and acidic deprotection of the product. Average radiochemical yield was 5%–10%, with a total synthesis time of 120 min. The specific activity of [^18^F]nifrolene was 74 GBq/μmol (2 Ci/μmol) at the end of synthesis, with a radiochemical purity of >98% after high-performance liquid chromatography purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20nifrolene%20and%20in%20vitro)]

Pichika et al. (7) reported that nifrolene, nifene, nifrolidine, 2-F-A83580, and nicotine had K_i_ values of 0.36, 0.50, 0.80, 1.33, and 2.83 nM, respectively, in [^3^H]cytisine or [^3^H]epibatidine (α4β2 nAchR) binding assays using rat brain membranes. In vitro autoradiography studies of rat brain slices indicated selective binding of [^18^F]nifrolene to thalamus > subiculum > striatum ≈ cortex > cerebellum, consistent with α4β2 receptor distribution. The thalamus/cerebellum, subiculum/cerebellum, and cortex/cerebellum rations were 9.3, 5.0, and 3.5, respectively. Nicotine (10 μM) blocked [^18^F]nifrolene-specific binding across the brain regions.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20nifrolene%20and%20rodentia)]

Pichika et al. (7) performed ex vivo biodistribution studies in rats after injection of 3.7 MBq (100 μCi) [^18^F]nifrolene (~10 ng). A peak uptake of 0.37% injected dose (ID)/g was reached in the thalamus at 60 min, followed by a gradual washout to 0.14% ID/g at 120 min. The thalamus/cerebellum ratio at 60 min was ~3. The cortex (0.25% ID/g) had a higher accumulation at 60 min than the cerebellum (0.12% ID/g). Pretreatment with nicotine (10 mg/kg, 5 min before tracer injection) decreased the thalamus/cerebellum ratio at 60 min to 1.8.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20nifrolene%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20nifrolene%20and%20%28primate%20not%20human%29)]

Pichika et al. (7) performed a biodistribution PET study in one anesthetized male rhesus monkey injected with 155 MBq (4.2 mCi) [^18^F]nifrolene. Their study showed accumulation of radioactivity in various regions of the brain, with the highest uptake in the regions of the anteroventral thalamic nucleus and thalamus, followed by lateral geniculate, cingulate gyrus, temporal cortex, and insular cortex. The monkey striatum and cerebellum showed lower binding than the other brain regions. The thalamus/cerebellum ratio peaked at 120 min after injection at a value of 1.7, whereas the cortex/cerebellum ratio was 1.3. [^18^F]Nifrolene exhibited faster binding kinetics than 2-[^18^F]FA, reaching a transient equilibrium within 2.5 h.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20nifrolene%20and%20human)]

No publication is currently available.

## NIH Support

R01 AG029479

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., Riganti L., Vailati S., Clementi F. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Ding Y.S., Fowler J.S., Logan J., Wang G.J., Telang F., Garza V., Biegon A., Pareto D., Rooney W., Shea C., Alexoff D., Volkow N.D., Vocci F. (2004). 6-[18F]Fluoro-A-85380, a new PET tracer for the nicotinic acetylcholine receptor: studies in the human brain and in vivo demonstration of specific binding in white matter. Synapse.
5 Kimes A.S., Horti A.G., London E.D., Chefer S.I., Contoreggi C., Ernst M., Friello P., Koren A.O., Kurian V., Matochik J.A., Pavlova O., Vaupel D.B., Mukhin A.G. (2003). 2-[18F]F-A-85380: PET imaging of brain nicotinic acetylcholine receptors and whole body distribution in humans. Faseb J.
6 Chattopadhyay S., Xue B., Collins D., Pichika R., Bagnera R., Leslie F.M., Christian B.T., Shi B., Narayanan T.K., Potkin S.G., Mukherjee J. (2005). Synthesis and evaluation of nicotine alpha4beta2 receptor radioligand, 5-(3'-18F-fluoropropyl)-3-(2-(S)-pyrrolidinylmethoxy)pyridine, in rodents and PET in nonhuman primate. J Nucl Med.
7 Pichika R., Kuruvilla S.A., Patel N., Vu K., Sinha S., Easwaramoorthy B., Narayanan T.K., Shi B., Christian B., Mukherjee J. (2013). Nicotinic alpha4beta2 receptor imaging agents. Part IV. Synthesis and biological evaluation of 3-(2-(S)-3,4-dehydropyrrolinyl methoxy)-5-(3'-(1)(8)F-fluoropropyl)pyridine ((1)(8)F-Nifrolene) using PET. Nucl Med Biol.